# [^11^C]N-Methyl-N-phenyl-[2-(4-chlorophenyl)-6,8-dichloroimidazo[1,2-a]pyridin-3-yl]acetamide

Chemical name: | [^11^C]N-Methyl-N-phenyl-[2-(4-chlorophenyl)-6,8-dichloroimidazo[1,2-a]pyridin-3-yl]acetamide
Abbreviated name: | [^11^C]PBR7
Synonym:
Agent category: | Compound
Target: | Peripheral-type benzodiazepine receptor (PBR), also known as translocator protein (TSPO)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Imidazopyridineacetamide)]

Benzodiazepines are potent psychoactive drugs used for their sedative and anxiolytic properties (1, 2). There are two types of benzodiazepine receptors, which have been designated as the central benzodiazepine receptors (CBRs) and peripheral benzodiazepine receptors (PBRs). The CBR is found exclusively in the central nervous system on the membranes of neurons and is coupled to the γ-aminobutyric acid receptor/chloride channel (3). In contrast, the PBR is a mitochondrial protein found in brain and peripheral tissues (adrenal gland, heart, lung, kidney, and testis) (4). The brain has lower levels of PBRs than do peripheral tissues. Both glial cells and macrophages contain high levels of PBRs (5-7). Increased PBR expression after brain injury or neuroinflammation is associated with microglial activation, such as occurs with the neuronal damage that accompanies several neurodegenerative diseases, including Alzheimer’s disease, Wernicke’s encephalopathy, multiple sclerosis, and epilepsy.

PBRs have been studied in vivo with positron emission tomography (PET) using 1-(2-chlorophenyl)-N-[^11^C]methyl-N-(1-methylpropyl)-3-isoquinoline carboxamide ([^11^C]PK11195), an isoquinoline carboxamide with specific PBR-antagonistic activity. [^11^C]PK11195 as been developed as a PET agent for non-invasive studies of microglia and macrophage activation in the brain, lung, and heart. However, accumulation of this tracer in the brain is limited. N-(2,5-Dimethoxybenzyl)-N-(5-fluoro-2-phenoxyphenyl)acetamide (DAA1106) has been found to be a selective agonist for studying PBRs in the central nervous system (8, 9). DAA1106 was reported to have a higher affinity for PBRs in mitochondrial fractions of rat and monkey brains than did PK11195 (8, 9). Therefore, both tracers are able to cross the normal cell membrane to reach the mitochondrial receptor sites. N-(5-Fluoro-2-phenoxyphenyl)-N-(2-[^18^F]fluoroethyl-5-methoxybenzyl)acetamide ([^18^F]FEDAA1106) and [^11^C]DAA1106 have been developed as potential PET ligands with highly selective and specific binding to PBR. [^11^C]N-Methyl-N-phenyl-[2-(4-chlorophenyl)-6,8-dichloroimidazo[1,2-a]pyridin-3-yl]acetamide ([^11^C]PBR7, a partial agonist) with an imidazopyridine acetamide structure has been developed for imaging PBR (10, 11).

### Related Resource Links:

- Chapters in MICAD (PBR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=PBR%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (PBR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=706%5Buid%5D))
- Articles in OMIM (PBR (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=109610))
- Clinical trials (PBR (http://www.clinicaltrials.gov/ct2/results?term=pk11195+OR+PBR))
- Drug information in FDA (PBR (http://google2.fda.gov/search?q=Peripheral-type+benzodiazepine+receptor+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=5&y=5))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Imidazopyridineacetamide%20and%20synthesis)]

Sekimata et al. (10) reported the synthesis of [^11^C]PBR7 by ^11^C-methylation of the N-desmethyl precursor with [^11^C]iodomethane in the presence of NaH in dimethylformamide for 3 min at 80ºC. [^11^C]PBR7 was purified with high-performance liquid chromatography. The specific activity was 20–150 GBq/μmol (0.54–4.05 Ci/μmol) with >98% radiochemical purity and a radiochemical yield of 36% (decay-corrected) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Imidazopyridineacetamide%20and%20in%20vitro)]

In vitro receptor binding studies showed that PBR7 had K_i_ values of 0.2 nM for PBR and >6,000 nM for CBR (11). PBR7 has a moderate lipophilicity (log P = 2.2). PK11195 exhibited a K_i_ value of 4.3 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Imidazopyridineacetamide%20and%20rodentia)]

Sekimata et al. (10) reported biodistribution studies of [^11^C]PBR7 in mice (n = 4 mice/group) that showed high accumulation of radioactivity in the lung (~22% injected dose (ID)/g), followed by the heart (~12% ID/g), spleen (~10% ID/g), kidney (10% ID/g), and liver (~7% ID/g) at 30 min after injection of 4 MBq (0.11 mCi) [^11^C]PBR7. Radioactivity levels peaked in most tissues during the first minute and subsequently declined to constant levels. In the brain, [^11^C]PBR7 exhibited the highest accumulation (~1.5% ID/g) in the cerebellum and olfactory bulbs at 60 min after injection, whereas the lowest accumulation was found in the thalamus and cortex (~0.8% ID/g). Co-injection of PK11195 and PBR7 (1 mg/kg) significantly decreased the accumulation (P < 0.05) in the heart, kidney, spleen, pancreas, and lung as well as in various brain regions at 30 min after injection. On the other hand, flumazenil (CBR antagonist) exhibited no inhibition in any examined tissue. Approximately 83% and >95% of radioactivity in the plasma and brain, respectively, was intact [^11^C]PBR7 at 30 min after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Imidazopyridineacetamide%20and%20%28dog%20or%20sheep%20or%20pig%20or%20rabbit%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Imidazopyridineacetamide%20and%20%28primate%20not%20human%29)]

No publications are currently available.

## Human Studies

[Pub Med (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Imidazopyridineacetamide%20and%20human)]

No publications are currently available.

## References

1 Mohler H., Okada T. (1977). Benzodiazepine receptor: demonstration in the central nervous system. Science.
2 Hunkeler W., Mohler H., Pieri L., Polc P., Bonetti E.P., Cumin R., Schaffner R., Haefely W. (1981). Selective antagonists of benzodiazepines. Nature.
3 Olsen R.W., Tobin A.J. (1990). Molecular biology of GABAA receptors. Faseb J.
4 Anholt R.R., Pedersen P.L., De Souza E.B., Snyder S.H. (1986). The peripheral-type benzodiazepine receptor. Localization to the mitochondrial outer membrane. J Biol Chem.
5 Jones H.A., Valind S.O., Clark I.C., Bolden G.E., Krausz T., Schofield J.B., Boobis A.R., Haslett C. (2002). Kinetics of lung macrophages monitored in vivo following particulate challenge in rabbits. Toxicol Appl Pharmacol.
6 Kuhlmann A.C., Guilarte T.R. (2000). Cellular and subcellular localization of peripheral benzodiazepine receptors after trimethyltin neurotoxicity. J Neurochem.
7 Zavala F., Lenfant M. (1987). Benzodiazepines and PK 11195 exert immunomodulating activities by binding on a specific receptor on macrophages. Ann N Y Acad Sci.
8 Okuyama S., Chaki S., Yoshikawa R., Ogawa S., Suzuki Y., Okubo T., Nakazato A., Nagamine M., Tomisawa K. (1999). Neuropharmacological profile of peripheral benzodiazepine receptor agonists, DAA1097 and DAA1106. Life Sci.
9 Chaki S., Funakoshi T., Yoshikawa R., Okuyama S., Okubo T., Nakazato A., Nagamine M., Tomisawa K. (1999). Binding characteristics of [3H]DAA1106, a novel and selective ligand for peripheral benzodiazepine receptors. Eur J Pharmacol.
10 Sekimata K., Hatano K., Ogawa M., Abe J., Magata Y., Biggio G., Serra M., Laquintana V., Denora N., Latrofa A., Trapani G., Liso G., Ito K. (2008). Radiosynthesis and in vivo evaluation of N-[11C]methylated imidazopyridineacetamides as PET tracers for peripheral benzodiazepine receptors. Nucl Med Biol.
11 Trapani G., Laquintana V., Denora N., Trapani A., Lopedota A., Latrofa A., Franco M., Serra M., Pisu M.G., Floris I., Sanna E., Biggio G., Liso G. (2005). Structure-activity relationships and effects on neuroactive steroid synthesis in a series of 2-phenylimidazo[1,2-a]pyridineacetamide peripheral benzodiazepine receptors ligands. J Med Chem.